# Gadolinium-diethylenetriamine pentaacetic acid-24-cascade-polymer

Chemical name: | Gadolinium-diethylenetriamine pentaacetic acid-24-cascade-polymer
Abbreviated name: | 24GdDTPACP
Synonym: | GdDTPA-cascade-24-polymer, Gd-DTPA-24-cascade-polymer, 24-gadolinium-DTPA-cascade-polymer, Gd-DTPA-24-cascade-polymer, Gd-DTPA-cascade-polymer
Agent category: | Macromolecule
Target: | Other
Target category: | Other – blood pool agent
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadolinium+24+cascade+polymer)]

Magnetic resonance imaging (MRI) delineates soft tissues by sampling the signal of tissue water protons to detect abnormalities in anatomy, pathology, and functionality in the human body. The imaging contrast, defined as the relative brightness of various parts of the body, is primarily determined by the tissue structures and the spin relaxation times of the water protons (the longitudinal relaxation time (T_1_) and the transverse relaxation time (T_2_)). Many physiological processes, including blood flow, diffusion, perfusion, and chemical exchange, also affect the imaging contrast. To improve the imaging contrast, a variety of experimental parameters can be optimized. Imaging contrast can be improved locally by using contrast agents specifically targeted to tissues and organs (1, 2). Blood pool agents are paramagnetic contrast agents designed to remain in the blood for a prolonged time compared to the conventional contrast agents like gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA). Blood pool agents are normally macromolecules attached gadolinium chelates or iron oxide nanoparticles (1). Their large size prevents them from diffusing through the endothelium of normal tissue and entering into interstitial space in detectable amounts before being completely excreted from body. In addition to the applications in magnetic resonance angiography (3-5), blood pool agents are used to target necrotic myocardium (6, 7), to access myocardial viability (8), and to detect various tumors (9, 10).

(GdDTPA)_24_-cascade-polymer is a synthetic polymeric gadolinium complex designed as a blood pool contrast agent for MRI (11, 12). The main molecular frame is a dendritic structure (dendrimer) built from a tri-mesoyl[benzene-1,3,5-tricarbonyl] core surrounded by two generations of 6 and 12 L-lysine residues. 24 Gd-DTPA moieties are covalently bound at the molecular surface (13). Each Gd-DTPA moiety contains lanthanide Gd(III) of high electron spin (7/2) and long electron relaxation time (14). Gd(III) forms a very stable complex with DTPA and leaves one structural water in rapid exchange with the bulk water of tissues. As a result, the T_1_ relaxation time of tissue water protons reduces significantly. Attaching Gd-DTPA to a macromolecule generates a field-dependent paramagnetic enhancement effect (PRE) (15, 16). The efficacy increases substantially as a result of the increase of the effective rotation correlation time τ_R_. The synthesis of dendrimer starts with formation of a core. Monomers are assembled radially according to certain dendritic rules and cascade to higher generations like a starburst. Dendrimers built in this way have a globular shape, which provides an open surface for attaching various species such as imaging agents and therapeutic drugs (13). As a carrier for MRI contrast agents, dendrimers possess a mono-dispersed, well-defined, and stable molecular structure with rigid branch segments, allowing the synthesis of paramagnetic particles with well-defined size and efficacy (13, 17).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium+24+cascade+polymer)+AND+synthesis)]

Nicolle et al. described a detailed synthesis of the dendritic backbone of free 24mer amine (18). First the monomer N,N’-(iminodi-2,1-ethandiyl)-bis[N2,N6-bis[(benzyloxy)carbonyl]-L-lysinamide) was prepared in a single step from commercially available starting materials. Three equivalents of the monomer were then reacted with the central core benzene-1,3,5-tricarbonyl trichloride to produce the benzyloxycarbonyl-protected 12mer amines with 80% yield. This precursor was converted to the free 12mer amine and subsequently treated with N_a_,N_t_-dibenzyloxy-carbonyl-L-lysine-p-nitrophenyl ester to produce the protected 24mer amine with >80% yield. The protected 24mer was further converted to the free 24mer amine (18). Coupling of a three-fold molar excess DTPA-ethyl ester with the free 24mer amine generated dendritic DTPA ligand, followed by complexation with Gd_2_O_3_ to form (GdDTPA)_24_-cascade-polymer.This compound has 24 GdDTPAs and the molecular mass is 17 kDa. Because the compound has a globular shape, the apparent molecular weight is 30–35 kDa (11, 12). (GdDTPA)_24_-cascade-polymer is commercially available (Schering AG, Berlin, Germany).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadolinium+24+cascade+polymer)+AND+(in+vitro))]

The in vitro T_1_ relaxivity of (GdDTPA)_24_-cascade-polymer was determined to be 11.9 mmol Gd^-1^ • s^-1^ at 0.47 T (20 MHz) at 40°C (12) and slightly decreased to 10 mmol Gd^-1^ • s^-1^ at 2 T (85 MHz) at 37°C (19). This relaxivity is two-fold higher than that of the single GdDTPA, which is 4.9 mmol Gd^-1^ • s^-1^ at 2 T (85 MHz) at 37°C (19).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadolinium+24+cascade+polymer)+AND+rodentia)]

The half-life time in rat plasma was measured to be 0.5 hr. Within 7 days, 99% of the agent was eliminated in the urine. The 50% lethal dose (LD_50_) was >30 mmol Gd/kg in the rat (12).

Schwickert et al. measured the MR angiographic properties of (GdDTPA)_24_-cascade-polymer (19). The peritumoral vessels were examined in rats bearing subcutaneous R32030 mammary adenocarcinomas on a 2-T MRI imager. At a dose of 0.05 mmol Gd/kg, (GdDTPA)_24_-cascade-polymer was used to effectively define the peritumoral vessels and the tumor rims. Su and colleagues performed a pharmacokinetic study of (GdDTPA)_24_-cascade-polymer in three animal tumor models in rats and mice (20). Dynamic contrast-enhanced MR imaging was used to examine the enhanced kinetics on a 1.5-T MRI imager. A dose of 0.07 mmol Gd/kg was administrated intravenously to rats bearing Walker 256 or R2320AC tumors and nude mice bearing human MCF7 carcinomas. The kinetic profiles suggested that (GdDTPA)_24_-cascade-polymer was predominately confined to the intravascular space. This low, whole-body distribution volume allowed for evaluation of the vascular volume, but its intermediate molecular size permitted a slow diffusion into the interstitial space through the vascular leakage and the rate of the leaking was used as the measure of vasculature permeability in tumors or other diseases. Roberts et al. used (GdDTPA)_24_-cascade-polymer to assess the acute or reperfused myocardial ischemia in rats because this type of contrast agent was more easily accumulated in the normal myocardium than in the ischemic region (20, 21). Dynamic, cardiac-gated, T_1_-weighted images were acquired on a 2-T MRI imager. The signal enhancement for the acute myocardial ischemia was found to be primarily located in normal myocardium but was negligible in ischemic myocardial muscle. The capillary permeability in the reperfused myocardial ischemia was found to have a five-fold increase compared to that of the normal myocardium. The temporal window available for imaging was ~18 min in rodents.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Adam et al. conducted signal enhancement measurement in the liver, renal cortex, pancreas, and trunk muscle of pigs at 1.5 T (11, 12). Five minutes after an i.v. injection of a dose of 0.05 mmol Gd/kg, 81% of the agent remained in the circulating blood. Signals in all organs peaked within 1 to 2 min and the enhancement lasted >30 min. The muscle was the only exception to have a slight signal enhancement compared to other organs such as liver, renal cortex, and pancreas. In a study of canine breast tumors in dogs at 1.5 T, a dose of 0.025 mmol Gd/kg was administrated to dogs that were diagnosed to have spontaneously occurring breast tumors 1.5–4.2 cm in diameter (22). The results showed that (GdDTPA)_24_-cascade-polymer allowed differentiation between benign and malignant breast lesions. Tacke et al. evaluated hypovascularized liver tumors (2–3 cm in diameter) in rabbits with a dose of 0.02 mmol Gd/kg (23). Single-slice, fast, low-angle shot (FLASH) gradient-echo images were collected on a 1.5-T MRI imager. Although the agents preceded a prolonged and incomplete distribution into the interstitial space of the tumor, the tumor remained hypointense, which yielded a marked contrast of tumor and liver tissue. The agents were eliminated from the body by glomerular filtration as the (GdDTPA)_24_-cascade-polymer.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadolinium+24+cascade+polymer)+AND+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadolinium+24+cascade+polymer)+AND+human)]

No publication is currently available.

## References

1 Weinmann H.J., Ebert W., Misselwitz B., Schmitt-Willich H. (2003). Tissue-specific MR contrast agents. Eur J Radiol.
2 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
3 Fink C., Goyen M., Lotz J. (2007). Magnetic resonance angiography with blood-pool contrast agents: future applications. Eur Radiol.
4 Kramer H., Morana G. (2007). Whole-body magnetic resonance angiography with blood-pool agents. Eur Radiol.
5 Hoffmann U., Schima W., Herold C. (1999). Pulmonary magnetic resonance angiography. Eur Radiol.
6 Kroft L.J., de Roos A. (1999). Blood pool contrast agents for cardiovascular MR imaging. J Magn Reson Imaging.
7 Muhler A. (1995). Assessment of myocardial perfusion using contrast-enhanced MR imaging: current status and future developments. Magma.
8 Schmiedl U., Moseley M.E., Sievers R., Ogan M.D., Chew W.M., Engeseth H., Finkbeiner W.E., Lipton M.J., Brasch R.C. (1987). Magnetic resonance imaging of myocardial infarction using albumin-(Gd-DTPA), a macromolecular blood-volume contrast agent in a rat model. Invest Radiol.
9 Kiessling F., Morgenstern B., Zhang C. (2007). Contrast agents and applications to assess tumor angiogenesis in vivo by magnetic resonance imaging. Curr Med Chem.
10 Daldrup H.E., Roberts T.P., Muhler A., Gossmann A., Roberts H.C., Wendland M., Rosenau W., Brasch R.C. (1997). , and , .
11 Adam G., Neuerburg J., Spuntrup E., Muhler A., Scherer K., Gunther R.W. (1994). Gd-DTPA-cascade-polymer: potential blood pool contrast agent for MR imaging. J Magn Reson Imaging.
12 Adam G., Neuerburg J., Spuntrup E., Muhler A., Scherer K., Gunther R.W. (1994). Dynamic contrast-enhanced MR imaging of the upper abdomen: enhancement properties of gadobutrol, gadolinium-DTPA-polylysine, and gadolinium-DTPA-cascade-polymer. Magn Reson Med.
13 Svenson S., Tomalia D.A. (2005). Dendrimers in biomedical applications--reflections on the field. Adv Drug Deliv Rev.
14 Weinmann H.-J., Brasch R.C. (1984). W.-R. Press, and G.E. Wesbey, Characteristics of gadolinium-DTPA complex: A potential NMR contrast agent. AJR.
15 Lauffer R.B. (1987). Paramagnetic metal complexes as water proton relaxation agents for NMR imaging:Theory and design. Chem. Rev.
16 Caravan P., Ellison J.J., McMurry T.J., Lauffer R.B. (1999). Gadolinium(III) Chelates as MRI Contrast Agents: Structure, Dynamics, and Applications. Chem Rev.
17 Wiener E.C., Brechbiel M.W., Brothers H., Magin R.L., Gansow O.A., Tomalia D.A., Lauterbur P.C. (1994). Dendrimer-based metal chelates: a new class of magnetic resonance imaging contrast agents. Magn Reson Med.
18 Nicolle G.M., Toth E., Schmitt-Willich H., Raduchel B., Merbach A.E. (2002). The impact of rigidity and water exchange on the relaxivity of a dendritic MRI contrast agent. Chemistry.
19 Schwickert H.C., Roberts T.P., Muhler A., Stiskal M., Demsar F., Brasch R.C. (1995). Angiographic properties of Gd-DTPA-24-cascade-polymer--a new macromolecular MR contrast agent. Eur J Radiol.
20 Su M.Y., Muhler A., Lao X., Nalcioglu O. (1998). Tumor characterization with dynamic contrast-enhanced MRI using MR contrast agents of various molecular weights. Magn Reson Med.
21 Roberts H.C., Saeed M., Roberts T.P., Muhler A., Brasch R.C. (1999). MRI of acute myocardial ischemia: comparing a new contrast agent, Gd-DTPA-24-cascade-polymer, with Gd-DTPA. J Magn Reson Imaging.
22 Adam G., Muhler A., Spuntrup E., Neuerburg J.M., Kilbinger M., Bauer H., Fucezi L., Kupper W., Gunther R.W. (1996). Differentiation of spontaneous canine breast tumors using dynamic magnetic resonance imaging with 24-Gadolinium-DTPA-cascade-polymer, a new blood-pool agent. Preliminary experience. Invest Radiol.
23 Tacke J., Adam G., Classen H., Muhler A., Prescher A., Gunther R.W. (1997). Dynamic MRI of a hypovascularized liver tumor model: comparison of a new blood pool contrast agent (24-gadolinium-DTPA-cascade-polymer) with gadopentetate dimeglumine. J Magn Reson Imaging.